# Radioiodinated anti-DNA-histone 1 complex chimeric tumor necrosis therapy (TNT) monoclonal antibody 1

Chemical name: | Radioiodinated anti-DNA-histone 1 complex chimeric tumor necrosis therapy (TNT) monoclonal antibody 1
Abbreviated name: | [^125/131^I]-chTNT-1
Synonym: | [^131^I]-chTNT; Cotara^®^
Agent Category: | Antibody
Target: | DNA-histone 1 complex
Target Category: | Nucleic acids-protein
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125/131^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=chTNT&cmd=DetailsSearch)]

Because neoplastic solid tumors grow rapidly, the lack of sufficient blood supply (and nutrition) leads to cell death and lysis in the lesion and results in the development and accumulation of necrotic areas in the affected areas. As a consequence of the lysis, the nuclear antigens (e.g., DNA, histone proteins, etc.) of the lysed cells are exposed in the necrotic tissues. Investigators have used the exposed antigens to develop monoclonal antibodies (mAbs) that have been radiolabeled for evaluation in preclinical and clinical studies to detect and treat malignant tumors (1). This treatment protocol is known as tumor necrosis therapy (TNT), and the mAb used for this treatment targets only the intracellular antigens present in the necrotic section of a tumor. Although the intact cell membrane of a viable cell does not allow the passage of mAbs (because of their large size), the lysed membrane of a necrotic cell provides mAbs with free access to bind the intracellular antigens, such as DNA-histone complexes, heterochromatic DNA, and single-strand DNA of the lysed cells (2). More than two decades ago, ^125^I-labeled F(ab’)_2_ fragments of a mAb designated TNT-1 were shown to bind the nuclear antigens of necrotic cells in xenograft tumors in nude mice. This observation was confirmed with gamma planar imaging using ^131^I-labeled TNT-1 F(ab’)_2_ fragments (3). In a subsequent study with nude mice bearing ME-180 cell tumors (of human cervical carcinoma origin), the intact [^131^I]-TNT-1 mAb was shown to have potential utility in the imaging and therapeutic treatment of the lesions, and it was concluded that treatment success was dependent on the number of necrotic cells present in the tumor (i.e., the higher the number of necrotic cells, the better the treatment results) (4). In another study, the TNT-1 mAb was determined to specifically target the histone H1 protein in nuclear extracts of Raji cells (5). Khawli et al. showed that uptake of the ^125^I-biotinylated chimeric TNT-1 mAb ([^125^I]-chTNT-1/B) by LS174T (human colon carcinoma cell line) and Madison 109 (murine adenocarcinoma cell line) cell tumors in mice was superior to that of the parent (non-biotinylated) [^125^I]-chTNT-1 mAb (2). Biotinylation was reported to improve uptake of the mAb by the tumor because it modified the surface charge, and reduced the circulation time of the molecule. In addition, conjugation of biotin to the mAb decreased the isoelectric point of the molecule and improved its pharmacokinetic properties (2). A ^111^In-labeled chimeric TNT-3 mAb (targets single-strand DNA), as well as its ^111^In-labeled Fab’ and F(ab’)_2_ fragments, were shown to be suitable for the detection of necrotic solid cancerous tumors in mice (6).

The mechanism of action of the radioiodinated TNT mAb is believed to be as follows: the mAb binds to the intracellular antigens present in the necrotic sections of a tumor, and the radioactive iodine bound to the mAb generates enough energy (as 90% β radiation (192 keV) and 10% γ radiation (364.5, keV)) to kill the surrounding tumor cells with little damage to the normal tissue (1). [^131^I]-chTNT-1/B mAb has also been evaluated in a phase I clinical trial for the treatment of advanced colon and colorectal cancers (7) and is under clinical evaluation for the treatment of high-grade adult gliomas (1). In 2003, the Chinese State Food and Drug Administration (CSFDA) approved the use of [^131^I]-chTNT-1/B mAb for the immunotherapy of advanced lung cancer in China (8).

### Related Resource Links

Clinical trials (http://clinicaltrials.gov/ct2/results?term=chTNT-1%2FB) with [^131^I]-chTNT-1/B

Modification of proteins PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Modification%20of%20proteins&cmd=DetailsSearch)

Antibody Biotinylation (http://www.ncbi.nlm.nih.gov/pubmed?db=pubmed&cmd=link&linkname=pubmed_pubmed&uid=20012818)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TNT-1%20mAb%20synthesis&cmd=DetailsSearch)]

TNT-1 mAbs used for the preclinical studies were purified from mouse ascites and radioiodinated (^125/131^I) with the Iodogen method as described by Epstein et al. (3). The specific activity of this preparation was reported to be 37 MBq/6.6 μmol (1 mCi/μmol) (4). The radiochemical yield (RCY) and radiochemical purity (RCP) of [^125/131^I]-TNT-1 mAb were not reported in these publications.

In another preclinical study, the source of chTNT was not reported; however, the RCY of the purified [^125^I]-chTNT-1/B was reported to be 90%–95%, and the RCP was >99% as determined with instant thin-layer chromatography (2). The specific activity of this labeled chimeric mAb was not reported. To study the biodistribution of [^125^I]-chTNT-1/B in rodents, the optimal mAb:biotin ratio for the molecule was determined to be 1:3 (2).

For clinical studies, chTNT was expressed in and purified from suspension cultures of NSO cells, a murine myeloma cell line, following good manufacturing practice procedures (1, 7, 8). The mAb was then biotinylated and labeled with ^131^I using the chloramine-T method as described elsewhere (2). The specific activity of [^131^I]-chTNT-1/B was reported to be ~370 GBq/6.6 μmol (10 Ci/6.6 μmol). The RCY and RCP of the labeled product were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TNT-1%20mAb%20in%20vitro&cmd=DetailsSearch)]

The isoelectric points of chTNT-1 and chTNT-1/B were determined to be >9.6 and 7.2–7.8, respectively (2). Using a radioimmunoassay with Raji cells, the affinity constants of the parent mAb and the biotinylated mAb were reported to be 2.5 nM and 2.0 nM, respectively (2).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TNT-1%20mAb%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^131^I]-TNT-1 was investigated in nude mice (n = 5 animals/group) bearing ME-180 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-33&Template=cellBiology) tumors as described by Chen et al. (4). A ^125^I-labeled mAb (Lym-1; binds the surface antigen of B-lymphocytes) that does not react with the intracellular antigens was used as a control. The animals were infused with a mixture of the radioiodinated mAbs (TNT-1/B plus Lym-1; route of administration not mentioned), and the mice were euthanized at various time points varying from 4 h to 8 days after the treatment. At each time point, the major organs were obtained from the animals and accumulated radioactivity was determined. In the organs and the tumors, similar biodistribution patterns were observed for both of the radioiodinated mAbs 1 week after administration of the labeled biomolecules. Repeat dosing of the mice (at 1 and 2 weeks after the initial dose), however, followed by gamma planar imaging of the animals 1 week after each dose, revealed that the amount of radioactivity from [^131^I]-TNT-1 mAb in the tumors had increased after each dose (i.e., the amount of label in the tumors at week 3 was greater than that at week 2, and the amount of label in the tumors at week 2 was greater than that at week 1). No such trend was apparent in the tumors of mice treated with the control radioiodinated mAb. From this study, the investigators concluded that the therapeutic efficacy of chTNT mAbs was dependent on the number of lysed cells present in the necrotic portion of a tumor (4). No blocking studies were reported.

In another study, the biodistribution and pharmacokinetics of [^125^I]-chTNT-1 and [^125^I]-chTNT-1/B were compared in nude mice (n = 4–5 animals/group) bearing LS174T cell tumors on the left flank (2). The animals were injected with the labeled mAbs through the tail vein and euthanized 1–3 days postinjection (p.i.) to determine the amount of radioactivity present in various organs and the tumors. Data obtained from this study were presented as percent injected dose per gram tissue (% ID/g). With [^125^I]-chTNT-1, the amounts of radioactivity in the blood, muscle, and tumor were 5.91 ± 0.40% ID/g, 0.37 ± 0.03% ID/g, and 2.78 ± 0.20% ID/g, respectively at 1 day p.i. With [^125^I]-chTNT-1/B, the accumulation of label in these organs was 2.53 ± 0.10% ID/g, 0.28 ± 0.04% ID/g, and 3.25 ± 0.36% ID/g, respectively, at 1 day p.i. The tumor/muscle (T/M) ratios for the non-biotinylated and the biotinylated mAbs at 1 day after treatment were 3.19 ± 0.15 and 4.27 ± 1.30, respectively (2). A similar trend for the T/M ratios was observed with both tracers at 3 days p.i. No blocking studies were reported. The circulation half-lives of [^125^I]-chTNT-1 and [^125^I]-chTNT-1/B were determined to be 30.40 ± 1.80 h and 17.4 ± 2.40 h, respectively (2).

From these studies, the investigators concluded that biotinylation of chTNT-1 improved its uptake by the tumors compared to the non-biotinylated mAb due to rapid clearance of the biotinylated mAb from circulation (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TNT-1%20mAb%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TNT-1%20mAb%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TNT-1%20mAb%20Human%20Studies&cmd=DetailsSearch)]

In a clinical trial, 107 patients were administered two doses of [^131^I]-chTNT-1/B either intravenously (i.v.; n = 62 patients with different cancers) or as an intratumoral injection (n = 45 patients with lung cancer) at 2- to 4-week intervals (9). Whole-body scintigraphic images of the individuals obtained at different time points varying from 0.5 h to 25 days after the treatment revealed retention of radioactivity in the vicinity of the tumors for at least 8 days and 25 days in patients who received the labeled mAb through the i.v. or the intratumoral route, respectively (9). During this study, the biodistribution of the label in the tumor and non-tumor areas was measured in 11 patients from each group. The average radiation dose absorbed by the tumor and the non-tumor lung tissue in patients who received the i.v. treatment was 8.45 Gy and 2.35 Gy, respectively, and the tumor/non-tumor (T/NT) ratio in these patients was 3.8. Patients who received the intratumoral treatment had radiation doses of 30.0 Gy and 2.65 Gy in the tumor and the non-tumor lung tissue, respectively, and the T/NT ratio in these patients was 16.1. Of the patients involved in this study (total 107 patients who received treatment either through i.v. or the intratumoral route), 3.7% (4 patients) showed a complete response (CR), 30.8% (33 patients) had a partial response (PR), 55.1% (59 patients) showed no change, and 10.3% (11 patients) showed progression of the disease. On the basis of this clinical trial, the CSFDA approved the use of [^131^I]-chTNT-1/B for the treatment of lung cancer in China.

In another clinical trial, 43 patients with advanced lung cancer were treated with two doses of [^131^I]-chTNT-1/B as described elsewhere (10). Among these patients, 22 individuals received the treatment as an i.v. infusion (Group 1), 16 were given an intratumoral injection of the labeled mAb (Group 2), and 5 patients received 75% of their dose as an i.v. infusion and 25% as an intratumoral injection (Group 3). Biodistribution of the label was investigated with scintigraphy in 39 of the 43 patients (4 individuals could not be evaluated), and the T/NT ratios of patients in the various groups were determined. The T/NT ratios of patients in Groups 1 (n = 19 individuals), 2 (n = 14 individuals), and 3 (n = 3 individuals) were 1.36, 14.6, and 9.38, respectively. At 4–6 days after treatment, background radioactivity was visible in the hearts, large blood vessels, and livers of the Group 1 patients, but little (in the liver and heart) or no tracer was visible in any organ of the Group 2 and 3 patients. Whole-body scintigraphy in a patient with non-small cell lung carcinoma at 1 day and 14 days after an intratumoral injection of [^131^I]-chTNT-1/B showed that the label was localized in and around the tumor during this period (10). In another patient who received the labeled mAb through an i.v. infusion, whole-body scintigraphy showed that the label was detected in the tumor 1 h after administration, but it was also detected in the heart at this time point. At 3 days and 6 days after treatment, the radioactivity in this patient was present mainly in the lung lesion and in a metastatic tumor of the leg. The response rate (CR + PR) of the patients in Groups 2 and 3 was 52.4% compared to 9.1% for the patients in Group 1. From this study, the investigators concluded that the intratumoral treatment route used with [^131^I]-chTNT-1/B was suitable for the treatment of late-stage lung cancer and probably also for the treatment of other cancerous tumors (10).

In a phase I clinical trial approved by the United States Food and Drug Administration (FDA), 21 patients with advanced colon or colorectal cancer were given an i.v. infusion of 12.95 to 66.23 MBq/kg (from 0.35 to 1.79 mCi/kg) [^131^I]-chTNT-1/B in cohorts of three individuals (7). Whole-body single-photon emission computed tomography (SPECT) imaging was performed on the patients at various time points ranging from 1 h to 6 days after treatment, and the dose uptake in tumors and the normal organs was calculated from the images for 12 patients as described by Street et al. (7). The radiation doses in these patients were <3.2 cGy/mCi and 0.726 cGy/mCi for the normal organs and the bone marrow, respectively. The tumors received an average dose of 12.6 ± 8.7 cGy/mCi, and the mean tumor dose was 616 cGy/mCi for individuals infused with 1.36 mCi/kg of the labeled mAb (n = 2 patients), 1,631 cGy/mCi for those treated with 1.57 mCi/kg (n = 3 patients), and 2,534 cGy/mCi for patients who received 1.79 mCi/kg (n = 3 individuals). The mean whole-body radiation dose (n = 12 patients) was 0.627 ± 0.270 cGy/mCi, and the blood clearance half-life and the whole-body effective half-life of [^131^I]-chTNT-1/B were 35.0 ± 9.1 h and 53.3 ± 17.1 h, respectively. Primary tumors were visible only in images obtained from patients who received a dose of >58.09 MBq/kg (1.57 mCi/kg) [^131^I]-chTNT-1/B, which was attributed to the availability of high amounts of the mAb (14–24 mg total dose) in these individuals (7).

The use of [^131^I]-chTNT-1/B has also been evaluated for the treatment of 51 patients with different types of malignant glioma in phase I and phase II clinical trials approved by the FDA (1, 11). Individuals enrolled in the study were treated with the radioiodinated mAb using the convection-enhanced delivery procedure that delivered [^131^I]-chTNT-1/B directly into the resection cavity as described elsewhere (11). In the phase I study, it was shown that a dose of >13,000 cGy could be delivered to the tumor, and the lesion retained 34 ± 9% of the dose at 24 h after treatment with a half-life of 46 ± 6 h. Magnetic resonance imaging and SPECT imaging of two patients showed that the labeled mAb was confined to the clinical targeted area of the glioma tumors in these individuals. In a subset of six malignant glioma patients in the phase II study, the local injection of 13.2–71.1 mCi radioactive [^131^I]-chTNT-1/B was calculated to produce an absorbed tumor dose of 5,492–13,573 cGy (11). A phase II clinical trial to confirm the dose of [^131^I]-chTNT-1/B required to treat glioblastoma multiforme at first relapse is currently in progress; no results have been published to date (1).

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## References

1 Hdeib A., Sloan A.E. (2011). Convection-enhanced delivery of 131I-chTNT-1/B mAB for treatment of high-grade adult gliomas. Expert Opin Biol Ther.
2 Khawli L.A., Mizokami M.M., Sharifi J., Hu P., Epstein A.L. (2002). Pharmacokinetic characteristics and biodistribution of radioiodinated chimeric TNT-1, -2, and -3 monoclonal antibodies after chemical modification with biotin. Cancer Biother Radiopharm.
3 Epstein A.L., Chen F.M., Taylor C.R. (1988). A novel method for the detection of necrotic lesions in human cancers. Cancer Res.
4 Chen F.M., Taylor C.R., Epstein A.L. (1989). Tumor necrosis treatment of ME-180 human cervical carcinoma model with 131I-labeled TNT-1 monoclonal antibody. Cancer Res.
5 Miller G.K., Naeve G.S., Gaffar S.A., Epstein A.L. (1993). Immunologic and biochemical analysis of TNT-1 and TNT-2 monoclonal antibody binding to histones. Hybridoma.
6 Khawli L.A., Alauddin M.M., Hu P., Epstein A.L. (2003). Tumor targeting properties of indium-111 labeled genetically engineered Fab' and F(ab')2 constructs of chimeric tumor necrosis treatment (chTNT)-3 antibody. Cancer Biother Radiopharm.
7 Street H.H., Goris M.L., Fisher G.A., Wessels B.W., Cho C., Hernandez C., Zhu H.J., Zhang Y., Nangiana J.S., Shan J.S., Roberts K., Knox S.J. (2006). Phase I study of 131I-chimeric(ch) TNT-1/B monoclonal antibody for the treatment of advanced colon cancer. Cancer Biother Radiopharm.
8 Wang H., Cao C., Li B., Chen S., Yin J., Shi J., Ye D., Tao Q., Hu P., Epstein A., Ju D. (2008). Immunogenicity of Iodine 131 chimeric tumor necrosis therapy monoclonal antibody in advanced lung cancer patients. Cancer Immunol Immunother.
9 Chen S., Yu L., Jiang C., Zhao Y., Sun D., Li S., Liao G., Chen Y., Fu Q., Tao Q., Ye D., Hu P., Khawli L.A., Taylor C.R., Epstein A.L., Ju D.W. (2005). Pivotal study of iodine-131-labeled chimeric tumor necrosis treatment radioimmunotherapy in patients with advanced lung cancer. J Clin Oncol.
10 Yu L., Ju D.W., Chen W., Li T., Xu Z., Jiang C., Chen S., Tao Q., Ye D., Hu P., Khawli L.A., Taylor C.R., Epstein A.L. (2006). 131I-chTNT radioimmunotherapy of 43 patients with advanced lung cancer. Cancer Biother Radiopharm.
11 Shapiro W.R., Carpenter S.P., Roberts K., Shan J.S. (2006). (131)I-chTNT-1/B mAb: tumour necrosis therapy for malignant astrocytic glioma. Expert Opin Biol Ther.